# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 scFv-human serum albumin

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 scFv-human serum albumin
Abbreviated name: | ^64^Cu-DOTA-T84.66 scFv-HSA
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8).

Single-chain variable fragments (scFvs) of mAbs with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) and the minibody fragment (a dimer of scFvs-C_H_3 with a linker comprising 18 amino acids; molecular mass = 80 kDa) of a murine/human chimeric anti-CEA T84.66 antibody have been evaluated for targeting in several tumor antigen systems with rapid tumor localization and high-contrast imaging (9, 10). In particular, murine/human chimeric anti-CEA T84.66 diabody and minbody, which retain excellent CEA-binding properties (dissociation constant = 0.01–0.6 nM) (11-13), were developed as CEA imaging agents. However, the pharmacokinetics of radiometal labeled antibodies, with high liver and kidney uptake, are generally not ideal for imaging (14). Albumin is known to accumulate in tumors (15) and has a long blood half-life (16). Furthermore, albumin fusion proteins have been shown to prolong the in vivo circulation of small peptides and proteins (17). A T84.66 single-chain antibody (scFv) was joined with human serum albumin (HSA) using recombinant technology to form T84.66 scFv-albumin fusion protein (T84.66 scFv-HSA), which was radiolabeled with ^64^Cu for localization of CEA-positive tumors in mice with positron emission tomography (PET) (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv%20+and%20synthesis)]

The recombinant T84.66 scFv-HSA was conjugated with N-hydroxysuccinimidyl-DOTA in a molar ratio of 1:17 (18). The DOTA-scFv-HSA (~1.8 nmol) was incubated with 32.56 MBq (1.85 mCi) of ^64^CuCl_2_ (pH, 5.5) at 43°C for 45 min. ^64^Cu-DOTA-T84.66 scFv-HSA was isolated with size-exclusion chromatography with a radiolabeling efficiency of ~100%. The specific activity was ~18.5 MBq/nmol (0.5 mCi/nmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv%20and%20in%20vitro)]

Radioimmunoreactivity of ^64^Cu-DOTA-T84.66 scFv-HSA for recombinant CEA was determined to be 87% with high-performance liquid chromatography analysis (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20rodentia)]

Yazaki et al. (18) performed a preliminary biodistribution study of ^64^Cu-DOTA-T84.66 scFv-HSA in a nude mouse with the use of a LS174T human colon carcinoma subcutaneous xenograft model. Data were obtained at 48 h after injection. Accumulation of the ^64^Cu-DOTA-T84.66 scFv-HSA in the CEA-expressing LS174T tumor was 32.3% injected dose (ID)/g. The tumor/blood and tumor/liver ratios were 9.8 and 2.4, respectively. PET imaging with the ^64^Cu-DOTA-T84.66 scFv-HSA was visualized at 4 h and reached the highest level at 24 h. There was relatively low radioactivity elsewhere (except the liver) in the mice, confirming the biodistribution data. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20human)]

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Fagerstam L.G., Frostell-Karlsson A., Karlsson R., Persson B., Ronnberg I. (1992). Biospecific interaction analysis using surface plasmon resonance detection applied to kinetic, binding site and concentration analysis. J Chromatogr.
12 Hefta L.J., Neumaier M., Shively J.E. (1998). Kinetic and affinity constants of epitope specific anti-carcinoembryonic antigen (CEA) monoclonal antibodies for CEA and engineered CEA domain constructs. Immunotechnology.
13 Williams L.E., Wu A.M., Yazaki P.J., Liu A., Raubitschek A.A., Shively J.E., Wong J.Y. (2001). Numerical selection of optimal tumor imaging agents with application to engineered antibodies. Cancer Biother Radiopharm.
14 Yazaki P.J., Wu A.M., Tsai S.W., Williams L.E., Ikler D.N., Wong J.Y., Shively J.E., Raubitschek A.A. (2001). Tumor targeting of radiometal labeled anti-CEA recombinant T84.66 diabody and t84.66 minibody: comparison to radioiodinated fragments. Bioconjug Chem.
15 Wang J., Ueno H., Masuko T., Hashimoto Y. (1994). Binding of serum albumin on tumor cells and characterization of the albumin binding protein. J Biochem.
16 Dennis M.S., Zhang M., Meng Y.G., Kadkhodayan M., Kirchhofer D., Combs D., Damico L.A. (2002). Albumin binding as a general strategy for improving the pharmacokinetics of proteins. J Biol Chem.
17 Dennis M.S., Jin H., Dugger D., Yang R., McFarland L., Ogasawara A., Williams S., Cole M.J., Ross S., Schwall R. (2007). Imaging tumors with an albumin-binding Fab, a novel tumor-targeting agent. Cancer Res.
18 Yazaki P.J., Kassa T., Cheung C.W., Crow D.M., Sherman M.A., Bading J.R., Anderson A.L., Colcher D., Raubitschek A. (2008). Biodistribution and tumor imaging of an anti-CEA single-chain antibody-albumin fusion protein. Nucl Med Biol.